# N-[^18^F]Fluoroethylpiperidin-4ylmethyl acetate

Chemical name: | N-[^18^F]Fluoroethylpiperidin-4ylmethyl acetate
Abbreviated name: | [^18^F]FEP-4MA
Synonym:
Agent category: | Compound
Target: | Acetylcholinesterase (AChE)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA)]

Acetylcholine is an endogenous neurotransmitter at cholinergic synapses and neuroeffector junctions in the peripheral and central nervous systems. It acts on nicotinic and muscarinic receptors to mediate complex functions, such as attention, memory, cognition, and consciousness. Degeneration of cholinergic neurons has been observed in several neurodegenerative diseases, such as Alzheimer’s disease (AD) and Parkinson’s disease (PD), but not in vascular dementia. Acetylcholinesterase (AChE) is the enzyme that terminates cholinergic actions through the rapid hydrolysis of acetylcholine to choline and acetate. AChE is localized on both cholinergic and cholinoceptive neurons in the brain, with the highest activity in the striatum, thalamus, cerebellum, and cerebral cortex (1). AChE has been a target for radioligand development as well as drug development because its levels decrease in AD (1, 2). Radiolabeled AChE inhibitors and acetylcholine analog substrates are the two major approaches to mapping AChE in vivo in the human brain.

For measurements of AChE activity, various labeled esters of 1-methy-4-hydroxypiperidine have been designed and evaluated as acetylcholine substrate analogs (3). One of these analogs, N-[^11^C]methylpiperidin-4-yl acetate ([^11^C]MP4A), was chosen for further development as a positron emission tomography (PET) radioligand (4). [^11^C]MP4A has a tertiary amine structure that makes it lipophilic, and thus it readily crosses the blood–brain barrier (BBB). [^11^C]MP4A is specifically hydrolyzed by AChE (99% specificity) and yields a hydrophilic metabolite, N-[^11^C]methylpiperidinol ([^11^C]MP4OH), which is trapped in the brain because it is too polar to cross the BBB. [^11^C]MP4A is being developed as a PET agent for the non-invasive study of brain AChE activity in patients with AD and PD. Because ^18^F, with a longer physical half-life, has an advantage over ^11^C, N-[^18^F]fluoroethylpiperidin-4ylmethyl acetate ([^18^F]FEP-4MA), an analog of [^11^C]MP4A, has been evaluated as a potential PET agent for AChE activity in the brain (5).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=AChE+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (AChE (http://www.ncbi.nlm.nih.gov/gene/43)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=100740)
- Clinical trials (AChE (http://www.clinicaltrials.gov/ct2/results?term=Acetylcholinesterase))
- Drug information in FDA (http://google2.fda.gov/search?q=Acetylcholinesterase+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=17)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA%20and%20synthesis)]

Kikuchi et al. (6) reported the synthesis of [^18^F]FEP-4MA by reacting piperidin-4-ylmethyl acetate with 1-bromo-2-[^18^F]fluoroethane in dimethylformamide, with a radiochemical yield of ~70% (end of synthesis) after purification with high-performance liquid chromatography. The radiochemical purity was >98% with a total synthesis time of 92–96 min from the end of bombardment. The specific activity of [^18^F]FEP-4MA was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA%20and%20in%20vitro)]

Kikuchi et al. (6) reported that [^18^F]FEP-4MA was rapidly hydrolyzed to [^18^F]FEP-MP4OH and acetic acid by rat cerebral cortical homogenate, with 86% specificity for AChE. The hydrolysis rate constant was 1.67 min^-1^, which is similar to that of [^11^C]MP4A.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA%20and%20rodentia)]

Kikuchi et al. (5) performed ex vivo biodistribution studies in rats, which showed rapid, high accumulation of radioactivity in various regions of the brain within minutes of injection with [^18^F]FEP-4MA. The uptake values in striatum, hippocampus, cortex, and cerebellum were ~1.6–2.0% injected dose/g (ID/g) at 1 min, reflecting known levels of AChE activity in the brain, with >90% of radioactivity in the form of [^18^F]FEP-4MOH. The retention fraction values were estimated from 1 min and 15 min after injection to be 0.65 and 0.45, respectively. The radioactivity levels in the blood and parietal bone were 0.4% ID/g and 0.3% ID/g at 30 min after injection, respectively. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEP-4MA%20and%20human)]

No publication is currently available.

## References

1 Shinotoh H., Fukushi K., Nagatsuka S., Irie T. (2004). Acetylcholinesterase imaging: its use in therapy evaluation and drug design. Curr Pharm Des.
2 Herholz K. (2003). PET studies in dementia. Ann Nucl Med.
3 Irie T., Fukushi K., Akimoto Y., Tamagami H., Nozaki T. (1994). Design and evaluation of radioactive acetylcholine analogs for mapping brain acetylcholinesterase (AchE) in vivo. Nucl Med Biol.
4 Irie T., Fukushi K., Namba H., Iyo M., Tamagami H., Nagatsuka S., Ikota N. (1996). Brain acetylcholinesterase activity: validation of a PET tracer in a rat model of Alzheimer's disease. J Nucl Med.
5 Kikuchi T., Okamura T., Zhang M.R., Fukushi K., Irie T. (2010). In vivo evaluation of N-[18F]fluoroethylpiperidin-4ylmethyl acetate in rats compared with MP4A as a probe for measuring cerebral acetylcholinesterase activity. Synapse.
6 Kikuchi T., Zhang M.R., Ikota N., Fukushi K., Okamura T., Suzuki K., Arano Y., Irie T. (2005). N-[18F] fluoroethylpiperidin-4ylmethyl acetate, a novel lipophilic acetylcholine analogue for PET measurement of brain acetylcholinesterase activity. J Med Chem.